# Ioxilan carbonate particles

Chemical name: | Ioxilan carbonate particles
Abbreviated name: | IX-C particles
Synonym: | Cyclic carbonate particles of ioxilan
Agent Category: | Compound
Target: | Reticuloendothelial system (RES) phagocytic cells
Target Category: | Phagocytosis
Method of detection: | Computed tomography (CT) and Planar X-ray
Source of signal: | Iodine (I)
Activation: | No
Studies: | - In vitro; - Rodents; - Non-primate non-rodent mammals

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28Ioxilan%20Carbonate%20particles%29%20OR%20%28cyclic%20carbonate%20of%20ioxilan%29)]

Ioxilan carbonate particles (IX-C particles) are X-ray contrast agent preparations developed for contrast enhancement of the liver in computed tomography (CT) imaging (1-3). Water-soluble, intravenous ioxilan injection is commercially (http://www.guerbet-us.com/page.php?name=products) available as an X-ray contrast agent for excretory urography and contrast enhanced computed tomographic (CECT) imaging of the head and body. However, IX-C as insoluble particles is not commercially available.

X-ray imaging (planar and tomographic) techniques depend on tissue density differences that provide the image contrast produced by X-ray attenuation between the area of interest and surrounding tissues (4). Contrast enhancement (opacification) with use of contrast agents increases the degree of contrast and improves the differentiation of pathologic processes from normal tissues. Because iodine, an element of high atomic density, causes high attenuation of X-rays within the diagnostic energy spectrum, water-soluble and reasonably safe iodinated contrast agents in intravenous injectable forms have been developed for clinical applications (5, 6). Water-soluble, intravenous X-ray contrast agents are generally organic iodine compounds that contain one or more tri-iodinated benzene rings. When injected intravenously, they are largely distributed in the extracellular fluid space and excreted unchanged by the kidneys. Contrast enhancement of a region of interest depends on the route of administration, delivery of the agent to the area by blood flow, and the final iodine concentration in the region (7, 8). There are two basic types of these compounds: ionic and nonionic agents (9).

Rapid i.v. injection of water-soluble X-ray contrast agents can be performed with dynamic computed tomography to improve the detectability of liver lesions (1-3). However, there are many limitations associated with this approach. Particulate contrast media have also been developed for selective opacification of the liver. This approach is based on the fact that particles are effectively taken up by the phagocytic cells (Kupffer cells) of the reticuloendothelial system (RES). Several particulate contrast agents have been developed. These particulate contrast agents can be classified into three groups: 1) emulsion of liposoluble oil; 2) encapsulation of water-soluble X-ray contrast agents in liposomes or polymeric microspheres; and 3) the lipophilic prodrugs derived from water-soluble contrast agents (1, 10). As a low-osmolar nonionic monomer, ioxilan was developed in an effort to increase the safety and tolerance of X-ray contrast agents (11, 12). The development of ioxilan was based on the belief that the introduction of a double methylene as a hydrophobic region and masking it with a hydrophilic hydroxyl group could lower the osmolality without adversely affecting the biological tolerance (13). Li et al. (1) prepared a biodegradable IX-C particle preparation based on the cyclic carbonate of ioxilan. IX-C particles serve as the prodrug of ioxilan that is targeted to the RES phagocytic cells. It is expected that IX-C particles are degraded inside the phagocytic cells to release the original nonionic, water-soluble ioxilan.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%28Ioxilan%20Carbonate%20particles%29%20OR%20%28cyclic%20carbonate%20of%20ioxilan%29%20%29AND%20synthesis)]

Li et al. (1) prepared IX-C particles by a solvent extraction/evaporation method. IX-C was initially prepared by mixing carbonyldiimidazole with ioxilan in dimethyl sulfoxide (DMSO) over a period of 30 min (14). The mixture was then stirred at 70 ºC overnight. A catalytic amount of sodium methoxide was added, and the reaction was terminated by diluting the DMSO with methylene chloride and washing with cold water. The yield of IX-C was 50%. IX-C obtained from this procedure was dissolved in methylene chloride and acetone (3:1 v/v). The IX-C solution was added to an aqueous solution of polyvinyl alcohol (PVA) and emulsified with a tissue homogenizer for 1 min. The mixture was then stirred at 400 rpm for 4 hrs. The resulting emulsion was centrifuged at 3,000 rpm, resuspended in distilled water, filtered by a 5-μm filter, and finally centrifuged again. This process was repeated three times to produce particles in the size between 0.36 to 5.54 μm (97%). For preparing particles with a narrower size distribution, the particles were separated further by density gradient centrifugation using colloidal suspension of silica (Percoll). These particles were suspended in a gradient system composed of pure water, 50% Percoll in water, and 100% Percoll. The suspension was centrifuged at 1,000 rpm for 10 min. The microparticles in the middle layer were in the size between 0.64 to 4.17 μm. These microparticles were washed three times in water by centrifugation (3,000 rpm for 10 min). When IX-C was dissolved in dimethylformamide and emulsified into an aqueous solution of PVA, IX-C nanoparticles in the size between 158 and 433 nm (97%) were formed. These particles were collected and washed with water by centrifugation at 10,000 rpm for 10 min.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%28Ioxilan%20Carbonate%20particles%29%20OR%20%28cyclic%20carbonate%20of%20ioxilan%29%20%29%20AND%20in%20vitro)]

Li et al. (1) used the scanning electron microscope and submicron particle analyzer to examine the IX-C microparticles. The microparticle preparation had an average diameter of 1-2 μm, and 95% are ranging between 0.6 and 2.0 μm. These particles were spherical with smooth surfaces, and the iodine content was 45%. In another similar study, Li et al. (3) reported that the IX-C nanoparticles had an average diameter of 290-300 nm

In a stability study of the IX-C microparticles (1), no immediate particle aggregation was observed when the microparticles were suspended in saline or in 0.1% Tween 80 solution. IX-C microparticles started to crumble and disintegrate after incubated in saline at 37 ºC for 2 wks. The particles were also stable when first mixed with the slightly acidic rat or rabbit plasma at 37 ºC. In 6 days, these particles were completely dissolved in plasma. The IX-C microparticles were completely dissolved in 0.1 N sodium hydroxide at 37 ºC within 1 h. Using reverse-phase high performance liquid chromatography (HPLC) analysis and Fast Atom Bombardment Mass spectroscopy, it was shown that the degradation of IX-C particles yielded ioxilan and carbon dioxide.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%28Ioxilan%20Carbonate%20particles%29%20OR%20%28cyclic%20carbonate%20of%20ioxilan%29%29%20AND%20rodentia)]

Acute toxicity studies of IX-C microparticles were tested in mice, and the median lethal dose was 3.1 g/kg (1.4 g I/kg) body weight for male and 2.6 g (1.2 g I/kg) for female (1). In a kidney toxicity study in rats, both IX-C microparticles and nanoparticles (100 mg/kg i.v. ) caused significant increases in blood urea nitrogen (BUN) and creatinine levels in one day after injection (2). These increases induced by IX-C nanoparticles were higher than those by microparticles. In rats injected with IX-C nanoparticles, histologic and microscopic studies of the kidneys revealed proximal tubule damages.

Li et al. (3) studied the biodistribution of IX-C microparticles and nanoparticles (50 mg I/kg) in rats. The tissue samples were analyzed by the inductively coupled plasma-mass spectrometry for iodine concentrations and HPLC for ioxilan concentrations. For IX-C nanoparticles, there was a substantial retention in the blood and liver after 5 min. The blood concentration was higher. Iodine levels in the live rand spleen remained unchanged for the next six h. There was a gradual decline in the liver concentration to about 10% of the injected dose at 24 h. There was also a decrease of iodine in the blood and a corresponding increase of iodine in the kidney. The iodine concentration the kidney increased to a peak at two h after administration. The kidney concentration decreased to a negligible level at 24 h. The blood kinetics of IX-C microparticles was similar to that of nanoparticles. Microparticles had a significantly lower liver concentration than that of nanoparticles, but the spleen concentration was significantly higher. The kidney uptake of IX-C or its degradation product of the nanoparticles was more than six times than that of the microparticles.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%28Ioxilan%20Carbonate%20particles%29%20OR%20%28cyclic%20carbonate%20of%20ioxilan%29%29%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

Li et al. (1) conducted CT imaging studies of IX-C microparticles in normal and VX2 liver tumor bearing rabbits. After i.v. doses of 100, 200, and 270 mg I/kg, the maximum liver attenuation enhancements (ΔHU) at 30 min after injection were 23, 38, and 110, respectively. At 200 mg I/kg, the ΔHU for the spleen was 245 immediately after injection. In the VX2 liver tumor rabbits, the tumors without contrast were barely detectable in all animals. After injection of 200 mg I/kg IX-C microparticles, the tumors were clearly visible for up to two h. There was an increase in the attenuation difference of 35 HU between the liver and the tumor.

In a kidney toxicity study, Li et al. (2) reported that the BUN and creatinine levels did not change significantly from levels before i.v. injection of 200 mg I/kg IX-C microparticles. No significantly lesions on the kidneys were observed.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%28Ioxilan%20Carbonate%20particles%29%20OR%20%28cyclic%20carbonate%20of%20ioxilan%29%29%20AND%20%28primate%20NOT%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%28Ioxilan%20Carbonate%20particles%29%20OR%20%28cyclic%20carbonate%20of%20ioxilan%29%29%20AND%20human)]

No publication is currently available.

## References

1 Li C., Kan Z., Yang D.J., Kuang L.R., Liu C.W., Wright K.C., Wallace S. (1994). Preparation, characterization, and evaluation of ioxilan carbonate particles for computed tomography contrast enhancement of liver. Invest Radiol.
2 Li C., McCuskey P., Yang D.J., Kan Z., Wallace S. (1996). Development of biodegradable ioxilan carbonate particles for contrast enhancement of the liver in computed tomography scanning: toxicity assessment. Acad Radiol.
3 Li C., Yu D., Kan Z., Yang D.J., Tansey W., Kuang L.R., Wallace S. (1996). Biodistribution of cyclic carbonate of ioxilan: a radiopaque particulate macrophage imaging agent. Acad Radiol.
4. Hoey, G.B. and K.R. Smith, Chemistry of X-ray contrast media, in Radiocontrast agents, M. Sovak, Editor. 1984, Springer-Verlag: New York. p. 23-125.
5 Wallingford V.H. (1953). The development of organic iodine compounds as x-ray contrast media. J Am Pharm Assoc Am Pharm Assoc (Baltim).
6. Swanson, D.P. and M.B. Alpern, Contrast media for computed tomography: Intravascular, intracavitary, xenon, reticuloendothelial, in Pharmaceuticals in medical imaging, D.P. Swanson, H. M. Chilton and J. H. Thrall, Editor. 1990, Macmillan Publishing Company: New York. p. 99-124.
7 Sovak M., Ranganathan R., Lang J.H., Lasser E.C. (1977). and Concepts in design of improved intravascular contrast agents. European Society of cardiovascular Radiology, Uppsala, (May): p. 25-27.
8 Almen T. (1969). Contrast agent design. Some aspects on the synthesis of water soluble contrast agents of low osmolality. J Theor Biol.
9 Almen T. Development of nonionic contrast media Invest Radiol 1985 20Suppl1 S2 9 2579043
10. Cheng, K.T. and S.E. Seltzer, Liposome-encapsulated contrast agents in diagnostic imaging, in Contrast Media: Biological Effects and Clinical Application, Z. Parvex, R. Moncada, and M. Sovak, Editors. 1987, CRC Press, Inc.: Boca Raton, Florida. p. 73-87.
11 Callantine M.R., Sovak M., Lu H.P. (1990). Ioxilan. Initial clinical observations. Invest Radiol.
12 Katzberg R.W., Donahue L.A., Morris T.W., Ventura J.A., Krutchen A.E., Proskin H.M., Sovak M., Cos L.R. (1990). Ioxilan, a third generation low osmolality nonionic contrast medium. Systemic and renal hemodynamic effects. Invest Radiol.
13 Sovak M. (1988). The need for improved contrast media. Ioxilan: updating design theory. Invest Radiol.
14 Kutney J.P., Ratcliffe A.H. (1975). A novel and mild procedure for preparation of cyclic carbonates: an excellent protecting group for vicinal diols. Synth. Commun.